# Gadolinium-Hexyl-1,4,7,10-tetraazacyclododecane-1,4,7-triacetic acid-progesterone

Chemical name: | Gadolinium-Hexyl-1,4,7,10-tetraazacyclododecane-1,4,7-triacetic acid-progesterone
Abbreviated name: | ProGlo, Gd-Hexyl-DO3A-Pro
Synonym:
Agent category: | Compound
Target: | Progesterone receptor (PR)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal: | Gadolinium (Gd3^+^)
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ProGlo)]

Estrogens and progesterones are endogenous hormones that produce many physiological effects (1). Estrogens act primarily by regulating gene expression. Estrogen receptors (ERs) are found in the cytoplasm and nucleus of cells in the female reproductive tract, breast, pituitary gland, hypothalamus, bone, liver, and other tissues, as well as in various tissues in men. Estrogens are lipophilic in that they enter the cell passively by diffusion through the cellular membrane. They bind to ERs in the cytoplasm and are transported to the nucleus.

Breast cancer is the most common malignancy in women. Approximately 33% of women who have this disease will die of disseminated breast cancer. The growth of breast epithelial cells is dependent on estrogen stimulation to induce progesterone receptor (PR) expression. Two-thirds of breast carcinomas express ERs. It has also been established that the ER status of the tumor is an important prognostic indicator in breast cancer (2). Women with ER-positive and PR-positive breast tumors have a better prognosis than women with ER-negative and PR-negative tumors in terms of responsiveness to anti-estrogen treatment. ER content in breast cancer has been assessed in vitro with receptor binding assays, which suffer from inter-assay variability and are also limited by intrinsic receptor heterogeneity of the primary and metastatic tumors. 16α-[^18^F]Fluoro-17β-estradiol ([^18^F]FES) has been proven to be a valuable tracer for studies of the ER status of primary and metastatic breast cancer (3). However, [^18^F]FES is cleared from the blood and metabolized in 20 min with only 20% of [^18^F]FES intact in a study with 15 breast cancer patients (4). Similarly, a [^18^F]-labeled progestin is also metabolized rapidly in humans (5). For magnetic resonance imaging (MRI), Sukerkar et al. (6) found that coupling of gadolinium-hexyl-1,4,7,10-tetraazacyclododecane-1,4,7-triacetic acid (Gd-hexyl-DO3A) to the C21 hydroxyl group of 21-hydroxylprogesterone renders the MRI probe (ProGlo) inaccessible for metabolism but still able to bind specifically to PR(+) breast cancer cells. ProGlo was shown to accumulate in PR-rich uterus and PR(+) tumors in vivo in mice.

### Related Resource Links:

- Chapters in MICAD (estrogen receptor (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=estrogen%20receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), progesterone receptor (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Progesterone%20receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (estrogen receptor (http://www.ncbi.nlm.nih.gov/gene/2099), progesterone receptor (http://www.ncbi.nlm.nih.gov/gene/5241))
- Articles in OMIM (estrogen receptor (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=133430), progesterone receptor (http://www.ncbi.nlm.nih.gov/omim/607311))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ProGlo%20AND%20synthesis)]

ProGlo was synthesized with alkylation of the 21-hydroxyl group of 21-hydroxylprogesterone by 1,6-dibromohexane (6). This biphasic alkylation reaction produced bromine-tethered progesterone in 74% yield. A coupling reaction with DO3A followed by insertion of the Gd^3+^ was performed with incubation with GdCl_3_ at 60°C with 58% yield. Gd-hexyl-DO3A and Gd-DO3A were also prepared as controls. The log P values were 1.40 ± 0.08, –1.21 ± 0.12, and –2.96 ± 0.35 for ProGlo, Gd-hexyl-DO3A, Gd-DO3A, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ProGlo%20AND%20in%20vitro)]

T1- and T2-Weighted MRI of ProGlo, Gd-hexyl-DO3A, and Gd-DO3A was performed at 1.4 T at 37°C (6). The r_1_ and r_2_ relaxivity values for ProGlo were 5.35 ± 0.74 mM^–1^s^–1^ and 6.14 ± 0.81 mM^–1^s^–1^, respectively. The r_1_ and r_2_ relaxivity values for Gd-hexyl-DO3A were 5.55 ± 0.22 mM^–1^s^–1^ and 6.38 ± 0.38 mM^–1^s^–1^, respectively. The r_1_ and r_2_ relaxivity values for Gd-DO3A were 4.05 ± 0.02 mM^–1^s^–1^ and 4.75 ± 0.35 mM^–1^s^–1^, respectively. ProGlo and Gd-hexyl-DO3A had similar relaxivities, which were higher than those of Gd-DO3A.

Cellular accumulation of ProGlo, Gd-hexyl-DO3A, and Gd-DO3A in PR(+) T47D and PR(–) MDA-MB-231 human breast tumor cells were measured at 1, 4, 10, and 24 h of incubation (6). Concentrations of Gd^3+^ were measured with inductively coupled plasma–mass spectrometry (ICP-MS). The accumulation of the lipophilic ProGlo was the highest in both cell types and was two-fold higher than Gd-hexyl-DO3A. Gd-DO3A showed only marginal accumulation because of its hydrophilic nature. The accumulation of ProGlo was higher in the T47D cells than in the MDA-MB-231 cells as ProGlo was retained longer inside the PR(+) cells due to PR binding. NO blocking studies were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ProGlo%20AND%20rodentia)]

Sukerkar et al. (6) performed ex vivo biodistribution studies of ProGlo (n = 5/group), Gd-hexyl-DO3A (n = 3/group), and Gd-DO3A (n = 5/group) in female CD-1 mice at 2, 6, and 24 h after intraperitoneal injection (0.15 mmol Gd/kg). ProGlo (Gd) accumulation measured with ICP-MS in the PR(+) tissues (the uterus (12 µg Gd/g), ovaries (5 µg Gd/g), and mammary glands (4 µg Gd/g)) was significantly higher than that of Gd-hexyl-DO3A and Gd-DO3A at 6 h after injection (P < 0.05). The ProGlo accumulation in the liver (>1,000 µg Gd/g) was higher than in the kidney (~10 µg Gd/g). Gd-Hexyl-DO3A exhibited ~25 µg Gd/g in the liver and kidney initially and declined thereafter. There was little accumulation in the PR(+) tissues at the time points studied. Gd-DO3A exhibited a low accumulation in the liver (10 µg Gd/g) but a higher accumulation in the kidney (100 µg Gd/g) at 2–6 h after injection. There was high accumulation in the PR(+) tissues (7–10 µg Gd/g) at 2 h; this accumulation declined to levels below those of ProGlo at 6 h. No apparent acute toxicity was observed at 24 h after injection. NO blocking studies were reported.

In vivo MRI studies in the uteri and ovaries of female CD-1 mice (n = 3/group) were performed at 0, 2, 6, and 24 h after injection (7.05 T) with intraperitoneal injection of ProGlo or Gd-DO3A (6). ProGlo exhibited a significant increase in the contrast/noise ratio (CNR) relative to the CNR before injection through 24 h after injection (P < 0.05) in the uteri, whereas the increase in CNR was not significant in the ovaries. No significant increases were observed with Gd-DOA3 in the uteri or ovaries. Ex vivo MRI of the uteri or ovaries were also performed. The tissues from mice injected with ProGlo showed increased signal intensity in the PR-rich myometrium and ovarian follicles compared with those injected with Gd-DOA3 and untreated mice.

In vivo MRI studies were performed in nude mice (n = 2–4/group) bearing PR(+) T47D tumor on the right rear flank and PR(–) MDA-MB-231 tumor on left rear flank after intraperitoneal or subcutaneous injection of ProGlo and Gd-DOA3 at 0, 2, 6, and 24 h after injection (7.05 T) (6). ProGlo significantly increased the CNR of PR(+) tumors compared with PR(–) tumors and pre-injection (P < 0.05) at 2 h and 6 h, whereas Gd-DOA3 showed no significant difference between the two tumors and pre-injection at 2 h and 6 h. Intraperitoneal and subcutaneous injection of ProGlo exhibited a similar increased tumor accumulation in the PR(+) tumors. However, subcutaneous injection showed less toxicity (death) than intraperitoneal injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ProGlo%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ProGlo%20AND%20primates%20not%20humans)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ProGlo%20AND%20human)]

No publication is currently available.

## NIH Support

R01 EB005866, R21 CA143331, P30 CA060553

## References

1 Beato M., Klug J. (2000). Steroid hormone receptors: an update. Hum Reprod Update.
2 Vollenweider-Zerargui L., Barrelet L., Wong Y., Lemarchand-Beraud T., Gomez F. (1986). The predictive value of estrogen and progesterone receptors' concentrations on the clinical behavior of breast cancer in women. Clinical correlation on 547 patients. Cancer.
3 Flanagan F.L., Dehdashti F., Siegel B.A. (1998). PET in breast cancer. Semin Nucl Med.
4 Mankoff D.A., Tewson T.J., Eary J.F. (1997). Analysis of blood clearance and labeled metabolites for the estrogen receptor tracer [F-18]-16 alpha-fluoroestradiol (FES). Nucl Med Biol.
5 Verhagen A., Studeny M., Luurtsema G., Visser G.M., De Goeij C.C., Sluyser M., Nieweg O.E., Van der Ploeg E., Go K.G., Vaalburg W. (1994). Metabolism of a [18F]fluorine labeled progestin (21-[18F]fluoro-16 alpha-ethyl-19-norprogesterone) in humans: a clue for future investigations. Nucl Med Biol.
6 Sukerkar P.A., MacRenaris K.W., Meade T.J., Burdette J.E. (2011). A steroid-conjugated magnetic resonance probe enhances contrast in progesterone receptor expressing organs and tumors in vivo. Mol Pharm.